# Ad5-(PSE-BC)-(GAL4-(VP16)_2_)-(GAL4)_5_-Fluc

Chemical name: | Ad5-(PSE-BC)-(GAL4-(VP16)_2_)-(GAL4)_5_-Fluc
Abbreviated name: | AdTSTA-FL
Synonym:
Agent category: | Protein (Virus)
Target: | Androgen receptor
Target category: | Receptor
Method of detection: | Optical imaging
Source of signal/contrast: | Luciferin
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AdTSTA-FL)]

Adenoviruses (Ads) comprise a non-enveloped icosahedral protein shell (capsid) 70–100 nm in diameter surrounding an inner vial genome core (1). Human Ads consist of 51 distinct serotypes that are classified into six subgroups (species) designated A–F (2). Some serotypes such as serotypes 2 (Ad2) and 5 (Ad5) of species C only induce a mild, non-oncogenic respiratory infection, making them suitable for development of Ad-based vaccines and gene delivery vehicles for systematic administration (1). Their core genome, a linear, double-stranded DNA of ~36 kb, contains five early transcription units (E1A, E1B, E2, E3, and E4), four intermediate units (IVA2, IX, VAI, and VAII), and one later transcription unit (2). The functions in the early transcription regions have been well identified,: E1A activates cell cycles and initiates DNA replication; E1B blocks apoptosis induced by E1A activity; E2 facilitates viral DNA replication; E3 modulates host immune responses; and E4 regulates DNA replication, mRNA transport, and apoptosis (3). As a gene delivery vehicle, the genome core in Ad2 or Ad5 is usually modified with recombinant transcription activators (RTAs), in which foreign DNA with a size of up to 7.5 kb can be inserted in the deleted E1 or E3 regions in the Ads (4). Such genetic modification can incorporate ligands that can recognize specific cellular receptors and/or block the adenoviral naïve receptor (coxsackie-adenovirus receptor (CAR)), so that their tissue specificity is enhanced significantly. For example, the gene for the androgen receptor (AR) regulates the growth of prostate epithelial cells, induces the expression of prostate-specific antigen (PSA), and controls the growth of prostate cancer in the early phase. The AR gene can be introduced to the adenoviral genome to target AR-responsive prostate cancer or metastasis (5). Furthermore, reporter genes such as firefly luciferase (Fluc) (6) can be included for in vivo imaging, or suicide genes such as herpes simplex virus type 1-thymidine kinase (HSV1-tk) can be used for therapeutic applications (7). As an oxygenase (Mw = 62 kDa), Fluc oxidizes the heterocyclic substrate D-luciferin to oxyluciferin injected into the body and emits light in the wavelength range of 400–620 nm (8).

The transcriptional activity of adenoviral genes can be amplified several orders of magnitude with the use of the GAL4-VP2 fusion protein, where GAL4 is a DNA-binding domain (147 amino acids) and VP2 is a two-tandem repeat of the herpes simplex virus VP16 acidic activation domain (78 amino acids) (9). The two-step transcriptional amplification (TSTA) system is a novel recombinant transcription activation approach for designing a PSA promoter/enhancer, which can provide as high as ~800-fold enhancement in transcription activity compared with its conventional analog (10, 11). The TSTA system is composed of two parts in general; i.e., an activator BC-VP2 that contains a PSA promoter with a duplicated ARE4 enhancer core (each core has four binding sites for AR) to control the expression of the chimeric protein GAL4-VP2 and provide cell-specific binding, and the reporter (GAL4)_5_-Fluc (G5-FL), which contains a reporter with five GAL4 repeats to generate a GAL4-responsive Fluc signal (6). The two parts are linked in a head-to-head orientation and are inserted into the E1 region of Ad5 to produce Ad5-(PSE-BC)-(GAL4-(VP16)_2_)-(GAL4)_5_-Fluc (AdTSTA-FL), an optical agent for imaging AR-responsive PSA. Such a construct can provide ~50-fold amplification (11) via two steps: the PSA regulates the expression of the potent transcription activator GAL4-VP2, which in turn activates a GAL4-responsive reporter Fluc. AdTSTA-FL can function effectively as a gene delivery vehicle and as a lymphotropic agent in prostate cancer and metastasis in vivo (6, 12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( AdTSTA-FL)+AND+synthesis%0D%0A)]

The preparation of AdTSTA-FL was conducted in several steps (5, 6, 10, 11, 13). The commercial plasmid pBS II SK+ was used as the starting baseline construct pPSE (11). A NotI-flanked PSA enhancer/promoter expression cassette derived from plasmid PSAR2.4k-PCPSA-P-Lux was inserted into the pPSE to produce PSE. The synthetic ARE4 element that contained four key ARE elements was used to generate a duplicated enhancer core (13). The insertion of this duplicated core (C) in the PSE replaced the sequence between -3935 and -2855 in the PSE to produce a plasmid vector PBC. Then a GAL-VP2 fragment was inserted into PBC followed by creation of a unique NotI site. A NotI fragment, which contained both the PBC promoter and GAL-VP2 gene, was excised from the obtained plasmid PBC-VP2 and cloned into the NotI site of G5-FL to generate the vector PBC-VP2G5-FL (10). A SalI-Notl fragment containing the PBC-VP2G5-FL fragment was derived from the resulting PBC-VP2G5-FL and excised by NotI and partial SalI digestion (5). The produced expression cassette PBC-VP2G5-FL was inserted into the SalI-NotI site of the commercial vector pShuttle, which was then incorporated into the commercial Ad vector AdEasy through homologous recombination to produce AdTSTA-FL (6). The virus was propagated in 293 cells, purified on a CsCl gradient, and titered with plaque assays on 293 monolayers.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( AdTSTA-FL)+AND+%22in+vitro%22)]

Zhang et al. examined the activity of AdTSTA-FL in vitro (5). Androgen-dependent prostate cancer cells (LNCaP) were infected with AdTSTA-FL and incubated up to 48 h. The cells were harvested and lysed for assaying activity. GAL4-VP2 and Fluc levels were enhanced significantly in the presence of the synthetic androgen agonist R1881, with a maximum enhancement at 48 h after transcription. Similar studies were conducted in other cells, including MCF7 cells (androgen-expressing breast cancer cells) and PC3 (androgen-negative prostate cancer cells), but only a low basal level of TSTA expression was observed and did not respond to R1881. Thus the AdTSTA-FL responded only to androgen-dependent prostate cancer cells. AdTSTA-FL displayed 10-fold more ligand-induced Fluc activity than the control, AdCMV-FL.

Sato et al. examined the specificity of AdTSTA-FL in vitro on the basis of the measurement of infectivity (6). A variety of cells were used in the study, including LNCaP and LPAC-4 cells, H157 and A549 cells (lung cancer), MCF7 cells, and HepG2 cells (liver cancer). The infectivity in these cells with respect to that in the Hela cells (cervical carcinoma) was evaluated on the basis of their viral DNA uptake, which was 1.7 for LNCaP, 1.6 for H157, 1.5 for MCF7, and 1.1 for LAPC-4 and HepG2. Then the activity of AdTSTA-FL was evaluated in several prostate cancer cell lines, including two androgen-responsive cells (LNCaP and LPAC-4) and two AR-negative cells (DU145 and PC3). With a dose of one plaque-forming unit (pfu, an infectious unit) per cell (1 multiplicity of infection (m.o.i)), the normalized Fluc activity was 4.4-fold lower in LPAC-4 than that in LNCaP, whereas the AR-negative cells exhibited negative results (i.e., ~500-fold lower activity). The luciferase activity in other cancer cells was also measured and normalized to the activity measured for LNCaP, and all had much lower activity: a reduction of 2.9-fold was found in A549, 12-fold in H157, 45-fold in HepG2, 60-fold in Hela, and 200-fold in MCF7.

Burton et al. assessed the accumulation of AdTSTA-FL in lymph nodes ex vivo (12). Mice (n = 3) were injected with 1 × 10^8^ pfu AdTSTA-FL in 20 μl phosphate-buffered saline at their forepaws. Their draining lymph nodes (the axillary and brachial nodes) were dissected 24 h after injection. The nodal capsules were disrupted for extraction of the adenoviral particles. The transduction luciferase activity was found in ipsilateral axillary and brachial lymph nodes but not in the contralateral nodes. The number of viral genomes transported to and retained in the brachial node was ~60,000 copies, which was equivalent to ~0.1% delivery efficiency. Burton et al. also examined the transverse of AdTSTA-FL to regional lymph nodes in the mouse prostate Pten tumor suppressor gene knockout model (Pten^-/-^). Ten-week-old Pten^-/-^ mice with enlarged carcinoma prostate glands were injected with 1 × 10^8^ pfu AdTSTA-FL on their dorsolateral lobe. One hour later, ~1% of injected AdTSTA-FL was found in the periaortic lumbar nodes, with a smaller amount in more distant mesenteric and renal lymph nodes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( AdTSTA-FL) +AND++rodentia)]

Sato et al. investigated the specificity of AdTSTA-FL in vivo (6). SCID mice (n = 4, ~25 g) were implanted with LAPC-4 xenografts, and the tumors were allowed to grow for 3 weeks. AdTSTA-FL at a dose of 10^7^ pfu in 10 μl was injected into each tumor. A cooled-charged-coupled device (CCD) camera was used to image the in vivo expression over a 22-d period. For each imaging session, the mice were intravenously injected with 150 mg/kg D-luciferin (200 μl). A robust signal was observed 4 d after injection of AdTSTA-FL. Compared with the injection of the control AdCMV-FL, the average activity was 110-fold higher. As a control, naïve mice were used for the study. A low signal appeared only in the lung 22 d after intravenous injection of AdTSTA-FL. The kinetics of the expression after intratumoral injection of AdTSTA-FL was examined with sequential images between day 5 and day 13. The AdTSTA-FL displayed 50- to 100-fold higher levels of Fluc activity than the AdCMV-FL, and both gradually decayed from day 7.

Burton et al. examined the movement of AdTSTA-FL to lymph nodes in vivo (12). SCID/Beige (natural killer–deficient) mice were implanted with LAPC-9-VEGF-C tumor cells in the right shoulder, and the tumors were allowed to grow to 1.5 cm in diameter. Tumor-bearing mice and naïve mice were injected with 1 × 10^8^ pfu AdTSTA-FL in 20 μl phosphate-buffered saline in their forepaw and imaged with a CCD camera 4 d later. In each imaging session, the mice received 150 mg/kg D-luciferin intraperitoneally 20 min before imaging. A clear Fluc signal was observed in the axillary region of the tumor-bearing mice but not in the naïve mice. Burton et al. further assessed the lymph node metastases in nodal lesions of various sizes (12). Mice (n = 6) bearing 1-cm LAPC-9-VEGF-C-GFP-RL tumors were used for the study of macroscopic nodal lesions. A strong signal was observed in the ipsilateral axilla of mice with an injection of 1 × 10^8^ pfu AdTSTA-FL in both paws. Mice with orthotopic implanted LAPC-9-VEGF-C-GFP-RL tumors were used to examine the extensive peritumoral lymphatics. Fifteen days after tumor implantation, the mice were injected with 1 × 10^8^ pfu AdTSTA-FL in both hind paws. An observable luciferase signal was found in the inguinal and periaortic region 4 d later. The regional lymph nodes were excised for histological analysis after imaging, which further confirmed the metastasis lesion (~250 μm) of tumors present in the lymph nodes. As a control, luciferase tagged Ads that used cytomegalovirus (CMV) as promoter (AdCMV-FL) were injected in the forepaw of tumor-bearing mouse. The bioluminescence images demonstrated high nonspecific signal at the site of injection (paw) and in the liver caused by the systemic circulation.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( AdTSTA-FL) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( AdTSTA-FL) +AND+human)]

No publication is currently available.

### NIH Support

CA 82214, CA 92131, CA 101904, CA 92865, GM 08652

## References

1 Douglas J.T. (2007). Adenoviral vectors for gene therapy. Mol Biotechnol.
2 Majhen D., Ambriovic-Ristov A. (2006). Adenoviral vectors--how to use them in cancer gene therapy?. Virus Res.
3 Kuhlmann K.F., Gouma D.J., Wesseling J.G. (2008). Adenoviral gene therapy for pancreatic cancer: where do we stand?. Dig Surg.
4 Nettelbeck D.M., Jerome V., Muller R. (2000). Gene therapy: designer promoters for tumour targeting. Trends Genet.
5 Zhang L., Johnson M., Le K.H., Sato M., Ilagan R., Iyer M., Gambhir S.S., Wu L., Carey M. (2003). Interrogating androgen receptor function in recurrent prostate cancer. Cancer Res.
6 Sato M., Johnson M., Zhang L., Zhang B., Le K., Gambhir S.S., Carey M., Wu L. (2003). Optimization of adenoviral vectors to direct highly amplified prostate-specific expression for imaging and gene therapy. Mol Ther.
7 Johnson M., Sato M., Burton J., Gambhir S.S., Carey M., Wu L. (2005). Micro-PET/CT monitoring of herpes thymidine kinase suicide gene therapy in a prostate cancer xenograft: the advantage of a cell-specific transcriptional targeting approach. Mol Imaging.
8 Paulmurugan R., Gambhir S.S. (2005). Firefly luciferase enzyme fragment complementation for imaging in cells and living animals. Anal Chem.
9 Sadowski I., Ma J., Triezenberg S., Ptashne M. (1988). GAL4-VP16 is an unusually potent transcriptional activator. Nature.
10 Zhang L., Adams J.Y., Billick E., Ilagan R., Iyer M., Le K., Smallwood A., Gambhir S.S., Carey M., Wu L. (2002). Molecular engineering of a two-step transcription amplification (TSTA) system for transgene delivery in prostate cancer. Mol Ther.
11 Iyer M., Wu L., Carey M., Wang Y., Smallwood A., Gambhir S.S. (2001). Two-step transcriptional amplification as a method for imaging reporter gene expression using weak promoters. Proc Natl Acad Sci U S A.
12 Burton J.B., Johnson M., Sato M., Koh S.B., Mulholland D.J., Stout D., Chatziioannou A.F., Phelps M.E., Wu H., Wu L. (2008). Adenovirus-mediated gene expression imaging to directly detect sentinel lymph node metastasis of prostate cancer. Nat Med.
13 Wu L., Matherly J., Smallwood A., Adams J.Y., Billick E., Belldegrun A., Carey M. (2001). Chimeric PSA enhancers exhibit augmented activity in prostate cancer gene therapy vectors. Gene Ther.